# ^89^Zr-N-Succinyldesferal-chimeric monoclonal antibody G250

Chemical name: | ^89^Zr-N-Succinyldesferalchimeric monoclonal antibody G250
Abbreviated name: | ^89^Zr-Df-cG250
Synonym:
Agent category: | Antibody
Target: | Carbonic anhydrase IX
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=94963095), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=125661057) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=55894&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about human carbonic anhydrase IX.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr-cG250)]

In a variety of solid tumors, hypoxia was found to lead to tumor progression and the resistance of tumors to chemotherapy and radiotherapy (1-3). Tumor oxygenation is heterogeneously distributed within human tumors (4). Hypoxia in malignant tumors is thought to be a major factor limiting the efficacy of chemotherapy and radiotherapy. It would be beneficial to assess tumor oxygenation before and after therapy to provide an evaluation of tumor response to treatment and an insight into new therapeutic treatments (5). Tumor oxygenation is measured invasively using computerized polarographic oxygen-sensitive electrodes, which is regarded as the gold standard (6). Functional and non-invasive imaging of intratumoral hypoxia has been demonstrated to be feasible for the measurement of tumor oxygenation (7).

Chapman proposed the use of 2-nitroimidazoles for hypoxia imaging (8). 2-Nitroimidazole compounds are postulated to undergo reduction in hypoxic condition, forming highly reactive oxygen radicals that subsequently bind covalently to macromolecules inside the cells (9). [^18^F]Fluoromisonidazole ([^18^F]FMISO) is the most widely used positron emission tomography (PET) tracer for imaging tumor hypoxia (7). Carbonic anhydrase (CA) IX is one of the most overexpressed genes in cells under hypoxic conditions (10). It is a transmembrane glycoprotein with CA activity in the extracellular domain, and it is found to be overexpressed in renal cell, cervical, lung, and colorectal tumors. Murine monoclonal antibody G250 against CA IX has been developed for in vitro and in vivo localization of CA IX in cells (11-13). G250 is found to bind to >94% of human clear-cell renal carcinoma. A murine-human chimeric G250 (cG250) has been generated to be less immunogenic in humans. ^124^I-cG250 has been evaluated as a PET imaging agent for renal cell carcinoma in mice (14) and patients (15). Brouwers et al. (16) explored the use of a ^89^Zr positron emitter (half-life, 3.27 days) to radiolabel cG250. ^89^Zr was conjugated to a bifunctional derivative of desferrioxamine B (Df) to cG250 for PET imaging of CA IX expression in tumors. ^89^Zr-Df-cG250 has been evaluated as a PET imaging agent for renal cell carcinoma in rats.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Carbonic%20anhydrase+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Carbonic anhydrase IX (http://www.ncbi.nlm.nih.gov/gene/55894))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=CA%20IX)
- Clinical trials (G250 (http://www.clinicaltrials.gov/ct2/results?term=G250))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr-cG250+synthesis)]

cG250 was coupled with N-SucDf via an amide linkage and labeled with ^89^Zr (16). Df-cG250 (2.4 nmol) was incubated with 165 MBq (4.5 mCi) ^89^Zr for 30 min at room temperature. ^89^Zr-Df-cG250 was purified by gel filtration. The radiochemical purity was >97% with >95% immunoreactivity. Maximum specific activity was 60 MBq/nmol (1.6 mCi/nmol). There was one N-SucDf group per cG250 molecule. ^89^Zr-Df-cG250 showed <10% loss of ^89^Zr in human serum for 4 d at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr-cG250+in+vitro)]

Lawrentschuk et al. (17) performed binding experiments with^124^I-cG250 in SK-RC-52 human renal carcinoma cells. The dissociation constant (K_d_ ) was found to be 2.2 nM with 400,000 antibody molecules per cell.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr-cG250+rodentia)]

Brouwers et al. (16) studied ex vivo biodistribution of ^89^Zr-Df-cG250 in nude rats (n = 8) bearing SK-RC-52 tumors at 72 h after injection. The tracer accumulation in the tumors was 5.0 ± 2.4% injected dose per gram (ID/g). The liver, spleen, lung, intestines, muscle, blood, and kidneys had lower radioactivity levels than the tumors. The radioactivity in the blood was ~1.6% ID/g, and the tumor/blood ratio was 3.1. ^111^In-DTPA-cG250 exhibited a similar biodistribution pattern with a tumor/blood ratio of 2.9. No blocking experiment was performed. PET imaging with the ^89^Zr-Df-cG250 showed localization of radioactivity to the tumors and the abdomen area in the rats at 48 h and 72 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr-cG250+(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr-cG250+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr-cG250+human)]

No publication is currently available.

## References

1 Serkies K., Jassem J. (2005). Chemotherapy in the primary treatment of cervical carcinoma. Crit Rev Oncol Hematol.
2 Vaupel P., Mayer A. (2005). Hypoxia and anemia: effects on tumor biology and treatment resistance. Transfus Clin Biol.
3 Rajendran J.G., Krohn K.A. (2005). Imaging hypoxia and angiogenesis in tumors. Radiol Clin North Am.
4 Vaupel P., Harrison L. (2004). Tumor hypoxia: causative factors, compensatory mechanisms, and cellular response. Oncologist.
5 Dehdashti F., Grigsby P.W., Mintun M.A., Lewis J.S., Siegel B.A., Welch M.J. (2003). Assessing tumor hypoxia in cervical cancer by positron emission tomography with 60Cu-ATSM: relationship to therapeutic response-a preliminary report. Int J Radiat Oncol Biol Phys.
6 Raleigh J.A., Dewhirst M.W., Thrall D.E. (1996). Measuring Tumor Hypoxia. Semin Radiat Oncol.
7 Foo S.S., Abbott D.F., Lawrentschuk N., Scott A.M. (2004). Functional imaging of intratumoral hypoxia. Mol Imaging Biol.
8 Chapman J.D. (1979). Hypoxic sensitizers--implications for radiation therapy. N Engl J Med.
9 Chapman J.D., Baer K., Lee J. (1983). Characteristics of the metabolism-induced binding of misonidazole to hypoxic mammalian cells. Cancer Res.
10 Loncaster J.A., Harris A.L., Davidson S.E., Logue J.P., Hunter R.D., Wycoff C.C., Pastorek J., Ratcliffe P.J., Stratford I.J., West C.M. (2001). Carbonic anhydrase (CA IX) expression, a potential new intrinsic marker of hypoxia: correlations with tumor oxygen measurements and prognosis in locally advanced carcinoma of the cervix. Cancer Res.
11 Lam J.S., Pantuck A.J., Belldegrun A.S., Figlin R.A. (2005). G250: a carbonic anhydrase IX monoclonal antibody. Curr Oncol Rep.
12 Oosterwijk E., Debruyne F.M. (1995). Radiolabeled monoclonal antibody G250 in renal-cell carcinoma. World J Urol.
13 Grabmaier K., Vissers J.L., De Weijert M.C., Oosterwijk-Wakka J.C., Van Bokhoven A., Brakenhoff R.H., Noessner E., Mulders P.A., Merkx G., Figdor C.G., Adema G.J., Oosterwijk E. (2000). Molecular cloning and immunogenicity of renal cell carcinoma-associated antigen G250. Int J Cancer.
14 Lawrentschuk, N., F.T. Lee, G. Jones, A. Rigopoulos, A. Mountain, G. O'Keefe, A.T. Papenfuss, D.M. Bolton, I.D. Davis, and A.M. Scott, Investigation of hypoxia and carbonic anhydrase IX expression in a renal cell carcinoma xenograft model with oxygen tension measurements and (124)I-cG250 PET/CT. Urol Oncol, 2009
15 Divgi C.R., Pandit-Taskar N., Jungbluth A.A., Reuter V.E., Gonen M., Ruan S., Pierre C., Nagel A., Pryma D.A., Humm J., Larson S.M., Old L.J., Russo P. (2007). Preoperative characterisation of clear-cell renal carcinoma using iodine-124-labelled antibody chimeric G250 (124I-cG250) and PET in patients with renal masses: a phase I trial. Lancet Oncol.
16 Brouwers A., Verel I., Van Eerd J., Visser G., Steffens M., Oosterwijk E., Corstens F., Oyen W., Van Dongen G., Boerman O. (2004). PET radioimmunoscintigraphy of renal cell cancer using 89Zr-labeled cG250 monoclonal antibody in nude rats. Cancer Biother Radiopharm.
17 Ahlskog J.K., Schliemann C., Marlind J., Qureshi U., Ammar A., Pedley R.B., Neri D. (2009). Human monoclonal antibodies targeting carbonic anhydrase IX for the molecular imaging of hypoxic regions in solid tumours. Br J Cancer.